# Gadolinium-Diethylenetriamine pentaacetic acid-poly(lactic-co-glycolic acid) microbubbles

Chemical name: | Gadolinium-Diethylenetriamine pentaacetic acid-poly(lactic-co-glycolic acid) microbubbles
Abbreviated name: | Gd-DTPA-PLGA, Gd-PLGA
Synonym:
Agent category: | Compound
Target: | Non-targeted
Target category: | Non-targeted
Method of detection: | Multimodality imaging: magnetic resonance imaging (MRI), ultrasound (US)
Source of signal: | Gadolinium (Gd), microbubbles
Activation: | No
Studies: | - In vitro; - Non-primate non-rodent mammals | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gd-DTPA%20PLGA)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the density of nuclear proton spins, the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide and other iron oxide formulations affect T2 primarily and lead to a decreased signal. On the other hand, paramagnetic T1 agents such as gadolinium (Gd^3+^) and manganese (Mn^2+^) accelerate T1 relaxation and lead to brighter contrast images.

Ultrasound is the most widely used imaging modality in clinical medicine (2) and its role in noninvasive molecular imaging is expanding with ligand-carrying microbubbles (3). Microbubbles are spherical cavities filled by a gas and encapsulated in a shell. The shells are made of phospholipids, surfactant, denatured human serum albumin, or synthetic polymer. Ligands and antibodies can be incorporated into the shell surface of microbubbles. Microbubbles are usually 1–8 μm in size and provide a strongly reflective interface and resonate to ultrasound waves. They are used as ultrasound contrast agents in imaging of inflammation, angiogenesis, intravascular thrombus, and tumors (4-6). They can also potentially be used for drug and gene delivery (7). Ao et al. (8) used poly(lactic-co-glycolic acid) (PLGA) as an encapsulating agent to form a multimodality imaging agent composed of gadolinium-diethylenetriamine pentaacetic acid (Gd-DTPA) (for MRI) and fluorocarbon-filled microbubbles (for ultrasound). Gd-DTPA-PLGA has been evaluated with in vivo imaging of the liver in rabbits, exhibiting enhanced MRI and ultrasound signals.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Gd-DTPA+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Clinical trials (Gd-DTPA (http://www.clinicaltrials.gov/ct2/results?term=Gd-DTPA))
- Drug information in FDA (Gd-DTPA (http://google2.fda.gov/search?q=Gd-DTPA&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gd-DTPA%20PLGA%20and%20synthesis)]

Gd-DTPA-PLGA microbubbles were prepared with a double-emulsion method as described by Ao et al. (8). Laser particle-size analysis showed that the mean diameter of the microbubbles in saline solution (10^8^ microbubbles/ml) was 1.47 ± 0.38 µm. The mean Gd concentration in the microbubbles was 25 ± 2 µg/mg.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gd-DTPA%20PLGA%20and%20in%20vitro)]

Longitudinal relaxation rates (ms^-1^) of Gd-DTPA-PLGA at 0, 0.025, 0.05, and 0.075 mM Gd-DTPA were 7.13, 19.14, 21.73, and 23.19, respectively, measured at 1.5 T (8). Echo signal was detected in solution containing Gd-DTPA-PLGA with ultrasound scans (10 MHz).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gd-DTPA%20PLGA%20and%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gd-DTPA%20PLGA%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

Ao et al. (8) performed in vivo ultrasound imaging in rabbits after injection of ~2 × 10^10^ Gd-DTPA-PLGA microbubbles/kg (100 mg/kg) via the ear vein. The liver was the region of interest (20 mm^2^). The echo intensities of the liver parenchyma were 16.2 ± 0.7, 25.2 ± 0.4, 24.9 ± 0.5, 24.1 ± 0.4, 23.6 ± 0.3, 21.9 ± 0.8, 20.1 ± 0.5, and 19.2 ± 1.5 at 0, 5, 10, 15, 20, 25, 30, and 35 min after injection, respectively. The echo intensity reached a maximum value at 5 min and thereafter decreased gradually. Increased echo intensities were observed in the hepatic artery, portal vein, and hepatic vein. T1-Weighted MRI imaging of the liver was performed at 0, 2, 15, 30, and 60 min after injection of Gd-DTPA-PLGA (200 mg/kg), and the signal intensities were 257 ± 15, 420 ± 32, 476 ± 42, 509 ± 42, and 411 ± 68, respectively. The microbubbles had no effect on the functions of the kidney and liver up to 30 days after injection.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gd-DTPA%20PLGA%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Gd-DTPA%20PLGA%20and%20human)]

No publication is currently available.

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Wells P.N. (2001). Physics and engineering: milestones in medicine. Med Eng Phys.
3 Liang H.D., Blomley M.J. (2003). The role of ultrasound in molecular imaging. Br J Radiol.
4 Klibanov A.L. (2005). Ligand-carrying gas-filled microbubbles: ultrasound contrast agents for targeted molecular imaging. Bioconjug Chem.
5 Lindner J.R. (2004). Microbubbles in medical imaging: current applications and future directions. Nat Rev Drug Discov.
6 Villanueva F.S., Wagner W.R., Vannan M.A., Narula J. (2004). Targeted ultrasound imaging using microbubbles. Cardiol Clin.
7 Dijkmans P.A., Juffermans L.J., Musters R.J., van Wamel A., ten Cate F.J., van Gilst W., Visser C.A., de Jong N., Kamp O. (2004). Microbubbles and ultrasound: from diagnosis to therapy. Eur J Echocardiogr.
8 Ao M., Wang Z., Ran H., Guo D., Yu J., Li A., Chen W., Wu W., Zheng Y. (2010). Gd-DTPA-loaded PLGA microbubbles as both ultrasound contrast agent and MRI contrast agent--a feasibility research. J Biomed Mater Res B Appl Biomater.